# Perfluoropropane-filled, sorbitan monostearate– and polyoxyethylene 40 stearate–shelled nanobubbles

Chemical name: | Perfluoropropane-filled, sorbitan monostearate– and polyoxyethylene 40 stearate–shelled nanobubbles
Abbreviated name: | PFC-S60-PEG40S-NB
Synonym: | Nanobubbles
Agent Category: | Lipids
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Ultrasound
Source of signal / contrast: | Nanobubbles
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=ultrasound+and+nanobubbles+and+imaging)]

Perfluoropropane (PFC)-filled, sorbitan monostearate (also known as Span 60 (S60))- and polyoxyethylene 40 stearate (PEG40S)-shelled nanobubbles (NB), abbreviated as PFC-S60-PEG40S-NB, is a non-targeted ultrasound contrast agent developed by Xing et al. for tumor imaging on the basis of enhanced permeability and retention effect of tumor vasculature (1).

Microbubble agents are the most common type of ultrasound contrast agents and also the only type of these agents to be approved by the United States Food and Drug Administration (2-4). These microbubbles are filled with air or with a water-insoluble gas such as octafluoropropane (C_3_F_8_), decafluorobutane, or sulfur hexafluoride (5). The microbubble shell, designed to prevent gas diffusion, can be made of lipids, denatured albumin, or polymers (5). Although microbubbles are highly echogenic, the efficiency of in vivo contrast enhancement is closely related to the microbubble size, surface charge, shell composition, surface architecture, and gas core, particularly in the context of passive targeting (1, 5, 6). In terms of size, the resonant frequency of a microbubble is directly dependent on its size, and the contrast enhancement is closely associated with the size variance among microbubbles (4, 6). Currently, microbubble-enhanced ultrasound imaging is used to image blood perfusion and to measure blood flow rate in the heart, liver, and other organs (2, 7, 8). The mean size of most microbubble contrast agents is less than or approximately equal to the size of red blood cells, although the shell thickness varies from 10 nm to 200 nm. Microbubbles with a diameter <10 µm exhibit effective flow similar to that of red blood cells in the vascular system.

Tumor vasculature is characterized by the presence of open pores (380–780 nm) (9, 10). In contrast to blood-pool microbubbles, nanobubbles can pass more efficiently through the pores and accumulate within tumors. Therefore, a better imaging contrast may be achieved. Xing et al. developed a biocompatible PFC-filled nanobubble contrast agent by ultrasonication of a mixture of S60 and PEG40S, followed by isolation of the nanobubble subpopulation from the parent suspensions (1). S60 formed a condensed monolayer to prevent PFC escape from the core, while PEG40S was incorporated into the nanobubble shell to serve as a steric stabilizer. PEG40S is known to be a biocompatible, degradable, and nontoxic surfactant that is widely used in food products and pharmaceuticals. This chapter describes the data obtained by Xing et al. with PFC-S60-PEG40S-NB (1).

### Related Resource Links:

- FDA alert on microbubble contrast agents (http://www.fda.gov/Drugs/DrugSafety/PostmarketDrugSafetyInformationforPatientsandProviders/ucm110260.htm)
- MICAD chapters on microbubble contrast agents (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Ultrasound+AND+micad%5bbook%5d+AND+table%5btype%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Clinical trials of microbubble contrast agents in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=microbubble)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20220227)]

Xing et al. first prepared the PFC-filled microbubble suspension with a surfactant shell and a PFC core (1). PFC at 99.99% purity is commercially available. The shell was made of S60 and PEG40S by dissolving them together in phosphate-buffered saline. The PFC core was generated with high-power tip sonication of the vesicle/micelle aqueous solution. Centrifugation at 20g (relative centrifuged field) for 1, 2, 3, or 5 min was then applied to remove the microbubbles and isolate the nanobubble subpopulation. The yield of nanobubbles was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20220227)]

Xing et al. characterized the parental microbubbles and the nanobubbles in vitro (1). Preparation of the microbubbles by sonication of the mixed surfactants resulted in a polydispersed suspension. The mean diameter of microbubbles was 1.1–2.0 µm with a bimodal distribution centered at 400–600 nm and 3–5 µm, respectively. Optical analysis confirmed the polydispersity and the bimodal distribution of the parental microbubbles.

Centrifugation at 20g for 1 min slightly decreased the mean size of microbubbles to 1.1 µm with a bimodal distribution similar to the parental suspension. Centrifugation for 2 min further reduced the mean size to 820 nm but gave a broad distribution peaked at 400–600 nm. Increasing the time to 3 min markedly decreased the mean size (to 490 nm) and distribution (<1 µm for most bubbles) of the bubbles, and very little precipitate was observed in the samples. However, increasing the time to 5 min did not lower the mean size further, instead resulting in the destruction of the bubbles as well as a decrease in the bubble concentration. The 3-min nanobubbles remained stable at 4ºC under a C_3_F_8_ atmosphere for ~2 weeks without significant variations in the bubble size or morphology. Zeta potentials of the nanobubbles obtained from 3-min and 5-min samples were −35.4 mV and −33.9 mV, respectively. The nanobubbles obtained from 3 min centrifugation were used for in vivo imaging.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20220227)]

Xing et al. evaluated the nanobubbles in New Zealand white rabbits (n = 4) by imaging the kidneys in power Doppler mode (1). Upon intravenous injection of the nanobubbles, marked and complete power Doppler enhancement occurred immediately throughout the renal parenchyma. The enhancement lasted >15 min, indicating that the nanobubbles are stable enough for clinical ultrasonic imaging. No adverse effects were observed during the experiments (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Xing Z., Wang J., Ke H., Zhao B., Yue X., Dai Z., Liu J. (2010). The fabrication of novel nanobubble ultrasound contrast agent for potential tumor imaging. Nanotechnology.
2 Qin S., Caskey C.F., Ferrara K.W. (2009). Ultrasound contrast microbubbles in imaging and therapy: physical principles and engineering. Phys Med Biol.
3 Wilson S.R., Greenbaum L.D., Goldberg B.B. (2009). Contrast-enhanced ultrasound: what is the evidence and what are the obstacles?. AJR Am J Roentgenol.
4 Furlow B. (2009). Contrast-enhanced ultrasound. Radiol Technol.
5 Sirsi S., Borden M. (2009). Microbubble Compositions, Properties and Biomedical Applications. Bubble Sci Eng Technol.
6 Stride E. (2009). Physical principles of microbubbles for ultrasound imaging and therapy. Cerebrovasc Dis.
7 Chadderdon S.M., Kaul S. (2010). Molecular imaging with contrast enhanced ultrasound. J Nucl Cardiol.
8 Fleischer A.C., Niermann K.J., Donnelly E.F., Yankeelov T.E., Canniff K.M., Hallahan D.E., Rothenberg M.E. (2004). Sonographic depiction of microvessel perfusion: principles and potential. J Ultrasound Med.
9 Fang, J., H. Nakamura, and H. Maeda, The EPR effect: Unique features of tumor blood vessels for drug delivery, factors involved, and limitations and augmentation of the effect. Adv Drug Deliv Rev, 2010
10 Greish K. (2007). Enhanced permeability and retention of macromolecular drugs in solid tumors: a royal gate for targeted anticancer nanomedicines. J Drug Target.